# Polyethylene glycol–coated gold nanoshells conjugated with anti-VCAM-1 antibody

AuNS-PEG-VCAM-1Ab

Chemical name: | Polyethylene glycol–coated gold nanoshells conjugated with anti-VCAM-1 antibody
Abbreviated name: | AuNS-PEG-VCAM-1Ab, AuNS-PEG-Ab
Synonym:
Agent category: | Antibody
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target category: | Receptor
Method of detection: | Ultrasound, photoacoustic tomography (PAT) imaging; optical, near-infrared (NIR) fluorescence
Source of signal: | Gold (Au)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gold%20nanoshells%20VCAM-1)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–650 nm) are used. Near-infrared (NIR) fluorescence (650–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive alternative to radionuclide imaging in small animals (4, 5).

Photoacoustic imaging (PAI) is an emerging hybrid biomedical imaging modality based on photoacoustic effects (6-9). In PAI, non-ionizing optical pulses are delivered into biological tissues. Some of the delivered energy is absorbed and converted into heat, leading to transient thermoelastic expansion and thus ultrasonic emission. The generated ultrasonic waves are then detected by ultrasonic transducers to form images. It is known that optical absorption is closely associated with physiological properties, such as hemoglobin concentration and oxygen saturation. As a result, the magnitude of the ultrasonic emission (i.e., photoacoustic signal), which is proportional to the local energy deposition, reveals physiologically specific optical absorption contrast and tissue structures. However, exogenous NIR contrast agents are necessary to overcome the intrinsic low tissue and hemoglobin absorption and the scattering of signal in tissue. On the other hand, these small molecules exhibit fast clearance, small optical absorption cross section, and non-targeted specificity. Therefore, there is a need for contrast agents with long blood circulation and targeted specificity.

Gold (Au) nanoparticles have been studied as molecular imaging agents because of their bright NIR fluorescence emission of 700–900 nm and low toxicity (10). They can be tuned to emit in a range of wavelengths by changing their sizes, shapes, and composition, thus providing broad excitation profiles and high absorption coefficients. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds for in vitro and in vivo studies. Use of Au nanoparticles has been approved by the United States Food and Drug Administration for the treatment of patients with rheumatoid arthritis. Au nanoparticles have been studied as contrast agents in X-ray/computed tomography, NIR optical coherence tomography, PAI, and photoacoustic tomography (PAT) (3). NIR Au nanocages (AuNCs) are biocompatible, have low toxicity, and are tunable to strong NIR absorption (11). They have an outer edge of ~50 nm and an inner edge of ~42 nm, with a wall thickness of ~4 nm. Yang et al. (12) performed PAT of the cerebral cortex of rats with polyethylene glycol–coated AuNCs (PEG-AuNCs) as an optical contrast agent. The investigators observed an enhanced optical contrast in the vasculature in the cerebral cortex. Song et al. (13) demonstrated the use of Au nanocages as a PAI probe for detection of sentinel lymph nodes in rats.

Endothelial cells are important cells in inflammatory responses (14, 15). Bacterial lipopolysaccharide, virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Emigration of leukocytes from blood is dependent on their ability to adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movement of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (16).

VCAM-1 is found in very low levels on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (16-20). VCAM-1 binds to the very late antigen-4 (VLA-4) integrin on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression is also induced by oxidized low-density lipoproteins under atherogenic conditions (21). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression to vulnerable plaques, which may erode and rupture. Rouleau et al. (22) developed gold nanoshells coated with polyethylene glycol (PEG) and anti-VCAM-1 antibody (AuNS-PEG-VCAM-1Ab) for use with in vivo PAT imaging of atherosclerotic plaques in mice.

### Related Resource Links:

- Chapters in MICAD (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=VCAM-1+AND+micad%5Bbook%5D), gold imaging (http://www.ncbi.nlm.nih.gov/books?term=Gold%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VCAM-1 (http://omim.org/entry/192225))
- Clinical trials (VCAM-1 (http://www.clinicaltrials.gov/ct2/results?term=VCAM-1), gold nanoparticles (http://www.clinicaltrials.gov/ct2/results?term=gold+AND+nanoparticles))
- Drug information in FDA (VCAM-1 (http://google2.fda.gov/search?q=VCAM-1&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=11), gold nanoparticles (http://google2.fda.gov/search?q=gold%2BAND%2Brheumatoid%2Barthritis&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gold%20nanoshells%20VCAM-1%20and%20synthesis)]

Rouleau et al. (22) reported the synthesis of AuNS by incubation of HAuCl_4_ (9.5 µM) and cobalt nanoparticles in degassed water with stirring for 10 min at 25°C. The mixture was exposed to ambient conditions to allow oxidation of cobalt nanoparticles as the AuNS formed. AuNS nanoparticles were isolated with ultracentrifugation. To prepare AuNS-PEG-VCAM-1Ab, a solution of bi-functional OPSS-PEG-NHS (2 kDa) and rat anti-mouse VCAM-1 antibody (eBioscience, clone 429) was incubated overnight at 4°C. The reaction was stopped by addition of water to an antibody concentration of 0.13 nM that was mixed with AuNS. The mixture was incubated overnight at 4°C. The final product, AuNS-PEG-VCAM-1Ab nanoparticles, was isolated with centrifugation and ultrafiltration. The AuNS-PEG-VCAM-1Ab solution had a maximum absorbance at 710 nm. The external diameter was 38.7 ± 1.9 nm, with a shell thickness of 4.5 ± 0.2 nm as determined with transmission electron microscopy. There were ~1,500 antibody molecules per AuNS-PEG-VCAM-1Ab. The number of Ab molecules per nanoparticles decreased by ~25% after storage for 3 months at 4°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gold%20nanoshells%20VCAM-1%20and%20in%20vitro)]

In vitro cellular accumulation assays of AuNS-PEG-VCAM-1Ab and AuNS-PEG were performed in 2H11 mouse endothelial cells before and after stimulation with TNFα (22)_._ Fluorescence confocal imaging showed that AuNS-PEG-VCAM-1Ab bound to the activated 2H11 cells with marginal binding to nonactivated 2H11 cells. AuNS-PEG exhibited little binding to both activated and nonactivated 2H11 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gold%20nanoshells%20VCAM-1%20and%20rodentia)]

Rouleau et al. (22) performed ex vivo optical projection tomography with the excised hearts and attached aortas of apolipoprotein E–deficient (apoE−^/^−) mice (n = 5) and normal mice (n = 6) after intravenous injection of AuNS-PEG-VCAM-1Ab. The aorta and aortic value regions (n = 3) were selected for region-of-interest (ROI) analysis. The ROI/background ratio was ~100% higher for the apoE−^/^− mice than normal mice (P < 0.01). In vivo PAT imaging was performed through the cardiac window for each apoE−^/^− mouse (n = 3) after injection of AuNS-PEG-VCAM-1Ab. A linear scan was performed at a rate of 2 Hz with a single ultrasound transducer. Laser illumination pulses (710 nm) were 10 ns long, with a repetition rate of 20 Hz. Photoacoustic and ultrasound images were acquired simultaneously for 2 h after AuNS-PEG-VCAM-1Ab injection. A good PAT contrast showed the presence of AuNS in the aortic arch region, which was confirmed with the ultrasound images. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gold%20nanoshells%20VCAM-1%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gold%20nanoshells%20VCAM-1%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gold%20nanoshells%20VCAM-1%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Choi H.S., Frangioni J.V. (2010). Nanoparticles for biomedical imaging: fundamentals of clinical translation. Mol Imaging.
4 Leung K., Chopra A., Shan L., Eckelman W.C., Menkens A.E. (2012). Essential parameters to consider for the characterization of optical imaging probes. Nanomedicine (Lond).
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Wang L.V., Hu S. (2012). Photoacoustic tomography: in vivo imaging from organelles to organs. Science.
7 Bednar B., Ntziachristos V. (2012). Opto-acoustic imaging of drug discovery biomarkers. Curr Pharm Biotechnol.
8 Razansky D., Deliolanis N.C., Vinegoni C., Ntziachristos V. (2012). Deep tissue optical and optoacoustic molecular imaging technologies for pre-clinical research and drug discovery. Curr Pharm Biotechnol.
9 Luke G.P., Yeager D., Emelianov S.Y. (2012). Biomedical applications of photoacoustic imaging with exogenous contrast agents. Ann Biomed Eng.
10 Chithrani B.D., Ghazani A.A., Chan W.C. (2006). Determining the size and shape dependence of gold nanoparticle uptake into mammalian cells. Nano Lett.
11 Yang X., Stein E.W., Ashkenazi S., Wang L.V. (2009). Nanoparticles for photoacoustic imaging. Wiley Interdiscip Rev Nanomed Nanobiotechnol.
12 Yang X., Skrabalak S.E., Li Z.Y., Xia Y., Wang L.V. (2007). Photoacoustic tomography of a rat cerebral cortex in vivo with au nanocages as an optical contrast agent. Nano Lett.
13 Song K.H., Kim C., Cobley C.M., Xia Y., Wang L.V. (2009). Near-infrared gold nanocages as a new class of tracers for photoacoustic sentinel lymph node mapping on a rat model. Nano Lett.
14 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
15 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
16 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
17 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
18 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
19 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
20 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
21 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
22 Rouleau L., Berti R., Ng V.W., Matteau-Pelletier C., Lam T., Saboural P., Kakkar A.K., Lesage F., Rheaume E., Tardif J.C. (2013). VCAM-1-targeting gold nanoshell probe for photoacoustic imaging of atherosclerotic plaque in mice. Contrast Media Mol Imaging.